# Radioiodinated N-(2-diethylaminoethyl)-6-iodoquinoxaline-2-carboxamide dihydrochloride salt

Chemical name: | Radioiodinated N-(2-diethylaminoethyl)-6-iodoquinoxaline-2-carboxamide dihydrochloride salt | [image]
Abbreviated name: | [^125^I]ICF01012, [^125^I]3 | [image]
Synonym: | [^131^I]ICF01012, [^131^I]3 | [image]
Agent Category: | Compounds | [image]
Target: | Melanin | [image]
Target Category: | Others | [image]
Method of detection: | Single-photon emission computed tomography (SPECT), planar imaging | [image]
Source of signal / contrast: | ^125^I | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Chemical structure of ICF01012 (1).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=benzamide+and+imaging+and+therapy)]

Radioiodinated N-(2-diethylaminoethyl)-6-iodoquinoxaline-2-carboxamide dihydrochloride salt, abbreviated as [^125/131^I]ICF01012 or [^125/131^I]3, is a quinoxaline benzamide (BZA) derivative that was synthesized for melanin-targeted radionuclide imaging and therapy of melanoma (1, 2).

BZA derivatives represent a versatile class of aromatic compounds that possess a common structure element of Ph-CONH(CH_2_)_m_NR_2_ (m = 1, 2) and exhibit comparable properties, including high and specific binding with melanin in melanoma cells and melanocytes (3-5). Some of these compounds, such as N-(2-diethylaminoethyl)-4-[^123^I]iodobenzamide ([^123^I]BZA) and [^123^I]-N-(2-diethylaminoethyl)-2-iodobenzamide ([^123^I]BZA2), have been successfully evaluated in melanoma patients, showing high sensitivity and selectivity in the detection of melanoma and its metastasis (6-9).

The promising results with [^123^I]BZA have prompted great efforts from several groups in screening BZA analogs (3, 10, 11). Among them is a group of investigators in France who synthesized a series of BZA derivatives via structure-activity studies (12, 13). On the basis of the structure of the lead agent [^123^I]BZA, they synthesized a group of spermidine BZA derivatives by replacing the diethylaminoethyl moiety in the BZA structure with a triamine (spermidine). Spermidine BZA derivatives exhibit high affinity for melanin comparable to that of [^123^I]BZA; however, these compounds exhibit less accumulation in tumors than [^123^I]BZA in animal models of melanoma (14). More recently, the investigators generated a class of heteroaromatic BZA analogs by incorporating the heteroaromatic structure in place of the benzene moiety to take advantage of the polycyclic aromatic compounds that display a strong affinity for melanin while keeping the lipophilic side chain (15). The heteroaromatic analogs, [^125^I]5a through [^125^I]5I (http://www.ncbi.nlm.nih.gov/books/NBK23457/), showed high specific and long-lasting uptake in the melanoma, which is favorable for combined imaging and therapy. At the same time, the investigators also identified a group of quinoxaline analogs; radioiodinated derivative 3 (ICF01012) is one of these compounds, which show the most favorable pharmacokinetic properties for radionuclide therapy (1, 2). The rapid and specific tumor uptake of quinoxaline compounds also suggests that they are potentially valuable for radionuclide imaging. For radiofluorination, ICF01012 was modified by incorporating 2- or 6-fluoropyridine in the N,N-diethylethylenediamine framework of ICF01012. This strategy allows nucleophilic heteroaromatic radiofluorination of corresponding halogeno- or nitro-precursors without the need for an additional electron-withdrawing substituent in the aromatic ring. Fluoropyridine was introduced on the tertiary amine either directly or in combination with various linkers, which resulted in a group of amide tracers, such as the agent [^18^F]44 (16). These derivatives showed favorable properties for combined radionuclide imaging (^18^F, ^125^I) and therapy (^131^I) of melanoma using a single chemical structure. The following is a list of some representative agents that were synthesized and tested by the investigators from the group in France.

BZA derivatives: [^125/123^I]BZA, [^125^I]BZA2, [^125^I]BZ18, and [^125^I]5a through [^125^I]5I; and quinoxaline derivatives: [^125/131^I]ICF01012 (or [^125/131^I]3), [^125^I]56, and [^18^F]44.

This chapter summarizes the data of imaging studies obtained with [^125^I]ICF01012 (1, 2).

### Related Resource Links:

Melanin-targeted imaging agents in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=melanin+AND+micad%5bbook%5d&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Benzamide derivatives in PubChem (http://www.ncbi.nlm.nih.gov/sites/entrez?db=pcsubstance&term=benzamide) Benzamide derivatives in clinical trials in ClinicalTrials.gov (http://clinicaltrials.gov/ct2/results?term=benzamide)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=ICF01012)]

The procedure to synthesize ICF01012 has been reported previously in several papers (1, 2). Radioiodinated [^125^I]ICF01012 and [^131^I]ICF01012 were prepared using an iododestannylation reaction with [^125^I]NaI and [^131^I]NaI, respectively. Bonnet-Duquennoy et al. reported a 68% radiochemical yield with a radiochemical purity >98% and a specific activity of 114 GBq/μmol (3.08 Ci/µmol) for [^131^I]ICF01012, and a 52% radiochemical yield with a radiochemical purity >99% and a specific activity of 95 GBq/μmol (2.57 Ci/µmol) for [^125^I]ICF01012 (1).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=ICF01012)]

Bonnet et al. analyzed the uptake of [^125^I]ICF01012 in four melanoma cell lines after incubation with the cells for 24 h (2). The cell uptake (% of total labels) was 0.4 ± 0.1 and 0.8 ± 0.1 for the amelanotic lines A375 and M3Dau, respectively, and 3.0 ± 0.2 and 14.2 ± 2.3 for the pigmented lines M4Beu and SKMel3, respectively. The difference was significant between amelanotic and pigmented lines as well as between the highly pigmented line M4Beu and the less pigmented line SKMel3. The cell uptake level correlated with the melanin content in cells (Pearson correlation factor 0.981; P < 0.0001).

Bonnet-Duquennoy et al. imaged the localization of ICF01012 with secondary ion mass spectrometry after incubation with the culture colony of B16F0 melanoma cells (1). Images showed that ICF01012 was colocalized with the melanin polymers in the B16F0 cells (1).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=ICF01012)]

Bonnet et al. first investigated the accumulation of [^125^I]ICF01012 in tumor-bearing Swiss nu/nu mice (n = 5–6 per tumor type) with scintigraphic imaging after intravenous injection of 3.7 MBq (0.1 Ci) [^125^I]ICF01012 (2). In pigmented tumor models, [^125^I]ICF01012 showed rapid systemic elimination with a whole-body uptake of <20% in mice bearing M4Beu tumors and <15% in mice bearing SKMel3 tumors 24 h after injection. The uptake levels at 3, 6, and 24 h after injection were 6.5 ± 2.9, 6.4 ± 2.8, and 2.9 ± 1.4% injected dose per gram tissue (ID/g) in M4Beu tumors and 24.2 ± 4.8, 26.8 ± 4.5, and 11.7 ± 1.6% ID/g in SKMel3 tumors, respectively. In parallel to higher melanin content in SKMel3 tumors than in M4Beu tumors, the uptake was greater in SKMel3 tumors than in M4Beu tumors (P = 0.02 at 24 h after injection). The signal of [^125^I]ICF01012 from non-pigmented A375 and M3Dau tumors was not detectable at 3 h, and the respective uptake levels were only 1.9 ± 0.5 and 1.8 ± 0.7% ID/g at 6 h after injection, indicating the background radioactivity level in amelanotic A375 and M3Dau tumors. The tumor uptake of [^125^I]ICF01012 positively correlated with the tumor melanin content (correlation Pearson factor: 0.89; P < 0.0001).

Maisonial et al. investigated the accumulation of [^125^I]ICF01012 in C57B16 mice bearing B16F0 melanoma (n = 3 mice) (16). Significant tumor accumulation was observed at 1 h, and the accumulation increased gradually to a maximum at 3–6 h and continued to be measurable for at least 5 days after injection. The tumor uptake levels were 21.8 ± 6.6, 26.3 ± 6.6, 29.6 ± 8.4, 28.0 ± 8.2, 12.3 ± 3.7, 7.3 ± 3.6, 3.4 ± 0.3, and 1.9 ± 0.4% ID/g 1, 3, and 6 h and 1, 3, 5, 7, and 10 days after injection.

Bonnet et al. examined the radiotherapy efficacy of [^131^I]ICF01012 on M3Dau, M4Beu, and SKMel3 xenografts from the day that tumors became palpable (2). For all models, untreated groups (n = 10 mice) were studied in the same conditions. Lugol’s iodine solution was added to the feed for all groups of mice to block the thyroid. For the M4Beu radiotherapy experiment (n = 6 mice), [^131^I]ICF01012 was administered intravenously on days 14 and 18 (2 × 18.5 MBq (2 × 0.5 mCi)). A significant growth inhibition phase (GIP) of the M4Beu tumors was observed for up to 25 days. The GIP doubling times were 11.8 ± 2.0 and 8.4 ± 1.7 days for treated and untreated tumors, respectively (P = 0.02). Because SKMel3 tumors had higher melanin content and also higher [^125^I]ICF01012 uptake, only one injection of 18.5 MBq (0.5 mCi) [^131^I]ICF01012 was given to mice on day 35 after cell inoculation when tumors were measurable. SKMel3 tumors treated with [^131^I]ICF01012 exhibited a significant GIP from day 4 to day 25. For 50% of the treated animals, GIP extended to 47 days after treatment and correlated with smaller tumors on the day of injection. These results indicate that [^131^I]ICF01012 significantly decreased SKMel3 growth with GIP doubling times of 10.8 ± 2.4 and 18.1 ± 3.3 days for untreated and treated animals (P = 0.003), respectively. Using the same protocol with one injection, no significant difference was observed in M3Dau tumor growth. The doubling time was 6.7 ± 0.2 days for both treated and untreated M3Dau tumors (P = 0.39). After therapy, no gross changes of the organs, including liver, lung, and kidneys, were observed in any experiment (data not shown).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Bonnet-Duquennoy M., Papon J., Mishellany F., Labarre P., Guerquin-Kern J.L., Wu T.D., Gardette M., Maublant J., Penault-Llorca F., Miot-Noirault E., Cayre A., Madelmont J.C., Chezal J.M., Moins N. (2009). Targeted radionuclide therapy of melanoma: anti-tumoural efficacy studies of a new 131I labelled potential agent. Int J Cancer.
2 Bonnet M., Mishellany F., Papon J., Cayre A., Penault-Llorca F., Madelmont J.C., Miot-Noirault E., Chezal J.M., Moins N. (2010). Anti-melanoma efficacy of internal radionuclide therapy in relation to melanin target distribution. Pigment Cell Melanoma Res.
3 Oltmanns D., Eisenhut M., Mier W., Haberkorn U. (2009). Benzamides as melanotropic carriers for radioisotopes, metals, cytotoxic agents and as enzyme inhibitors. Curr Med Chem.
4 Chehade F., De Labriolle-Vaylet C., Michelot J., Moins N., Moreau M.F., Hindie E., Papon J., Escaig F., Galle P., Veyre A. (2001). Distribution of I-BZA (N-2-diethylaminoethyl-4-iodobenzamide) in grafted melanoma and normal skin: a study by secondary ion mass spectroscopy. Cell Mol Biol (Noisy-le-grand).
5 Greguric I., Taylor S.R., Denoyer D., Ballantyne P., Berghofer P., Roselt P., Pham T.Q., Mattner F., Bourdier T., Neels O.C., Dorow D.S., Loc'h C., Hicks R.J., Katsifis A. (2009). Discovery of [18F]N-(2-(diethylamino)ethyl)-6-fluoronicotinamide: a melanoma positron emission tomography imaging radiotracer with high tumor to body contrast ratio and rapid renal clearance. J Med Chem.
6 Bacin F., Michelot J., Bonafous J., Veyre A., Moreau M.F., Kemeny J.L., Chossat F., Bekhechi D. (1998). Clinical study of [123I] N-(2-diethylaminoethyl)-4-iodobenzamide in the diagnosis of primary and metastatic ocular melanoma. Acta Ophthalmol Scand.
7 Michelot J.M., Moreau M.F., Veyre A.J., Bonafous J.F., Bacin F.J., Madelmont J.C., Bussiere F., Souteyrand P.A., Mauclaire L.P., Chossat F.M., et al. (1993). Phase II scintigraphic clinical trial of malignant melanoma and metastases with iodine-123-N-(2-diethylaminoethyl 4-iodobenzamide). J Nucl Med.
8 Mansard S., Papon J., Moreau M.F., Miot-Noirault E., Labarre P., Bayle M., Veyre A., Madelmont J.C., Moins N. (2005). Uptake in melanoma cells of N-(2-diethylaminoethyl)-2-iodobenzamide (BZA2), an imaging agent for melanoma staging: relation to pigmentation. Nucl Med Biol.
9 Moins N., D'Incan M., Bonafous J., Bacin F., Labarre P., Moreau M.F., Mestas D., Noirault E., Chossat F., Berthommier E., Papon J., Bayle M., Souteyrand P., Madelmont J.C., Veyre A. (2002). 123I-N-(2-diethylaminoethyl)-2-iodobenzamide: a potential imaging agent for cutaneous melanoma staging. Eur J Nucl Med Mol Imaging.
10 Labarre P., Papon J., Moreau M.F., Moins N., Bayle M., Veyre A., Madelmont J.C. (2002). Melanin affinity of N-(2-diethylaminoethyl)-4-iodobenzamide, an effective melanoma imaging agent. Melanoma Res.
11 Moins N., Papon J., Seguin H., Gardette D., Moreau M.F., Labarre P., Bayle M., Michelot J., Gramain J.C., Madelmont J.C., Veyre A. (2001). Synthesis, characterization and comparative biodistribution study of a new series of p-iodine-125 benzamides as potential melanoma imaging agents. Nucl Med Biol.
12 Desbois N., Gardette M., Papon J., Labarre P., Maisonial A., Auzeloux P., Lartigue C., Bouchon B., Debiton E., Blache Y., Chavignon O., Teulade J.C., Maublant J., Madelmont J.C., Moins N., Chezal J.M. (2008). Design, synthesis and preliminary biological evaluation of acridine compounds as potential agents for a combined targeted chemo-radionuclide therapy approach to melanoma. Bioorg Med Chem.
13 Labarre P., Papon J., Rose A.H., Guerquin-Kern J.L., Morandeau L., Wu T.D., Moreau M.F., Bayle M., Chezal J.M., Croisy A., Madelmont J.C., Turner H., Moins N. (2008). Melanoma affinity in mice and immunosuppressed sheep of [(125)I]N-(4-dipropylaminobutyl)-4-iodobenzamide, a new targeting agent. Nucl Med Biol.
14 Moreau M.F., Papon J., Labarre P., Moins N., Borel M., Bayle M., Bouchon B., Madelmont J.C. (2005). Synthesis, in vitro binding and biodistribution in B16 melanoma-bearing mice of new iodine-125 spermidine benzamide derivatives. Nucl Med Biol.
15 Chezal J.M., Papon J., Labarre P., Lartigue C., Galmier M.J., Decombat C., Chavignon O., Maublant J., Teulade J.C., Madelmont J.C., Moins N. (2008). Evaluation of radiolabeled (hetero)aromatic analogues of N-(2-diethylaminoethyl)-4-iodobenzamide for imaging and targeted radionuclide therapy of melanoma. J Med Chem.
16 Maisonial A., Kuhnast B., Papon J., Boisgard R., Bayle M., Vidal A., Auzeloux P., Rbah L., Bonnet-Duquennoy M., Miot-Noirault E., Galmier M.J., Borel M., Askienazy S., Dolle F., Tavitian B., Madelmont J.C., Moins N., Chezal J.M. (2011). Single photon emission computed tomography/positron emission tomography imaging and targeted radionuclide therapy of melanoma: new multimodal fluorinated and iodinated radiotracers. J Med Chem.